# ^131^I-Labeled [Z]-2-[4-(1,2-diphenyl-1-di-butenyl)-phenoxy]-N,N-dimethylethanamine

Chemical name: | ^131^I-Labeled [Z]-2-[4-(1,2-diphenyl-1-di-butenyl)-phenoxy]-N,N-dimethylethanamine
Abbreviated name: | ^131^I-TAM
Synonym: | Tamoxifen
Agent Category: | Compound
Target: | Estrogen receptor (ER)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the structure of ^131^I-Tamoxifen for more information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tamoxifen+cancer)]

Tamoxifen (http://www.cancer.gov/cancertopics/druginfo/tamoxifencitrate) ([Z]-2-[4-(1,2-diphenyl-1-di-butenyl)-phenoxy]-N,N-dimethylethanamine (TAM)) is the first selective estrogen receptor (ER) modulator with extensive investigation for its anticancer properties (1, 2). The ^131^I-labeled form of TAM (^131^I-TAM) was developed to study the tumor response to antiestrogenic treatment and the ER expression in tumors and critical normal tissues (3).

TAM as first approved by the United States Food and Drug Administration (http://www.fda.gov/ohrms/dockets/ac/06/briefing/2006-4248B1-01-FDA-Tamoxifen Background Summary Final.pdf) in the 1970s for use in breast cancer treatment. Currently, it is widely used for the treatment of both early and advanced ER-positive breast cancer, as well as for the prevention of breast cancer in high-risk women (1, 4, 5). TAM itself is a prodrug, having relatively little affinity to ER. It is metabolized in the liver, mainly by the CYP2D6 and CYP3A4 enzymes (5, 6). Active metabolites such as 4-hydroxytamoxifen and N-desmethyl-4-hydroxytamoxifen have 30–100 times more affinity with the ER than TAM itself. These metabolites compete with estrogen for binding to ER and form a nuclear complex that inhibits DNA synthesis and blocks estrogen effects (5, 6). As a result, tumor cells stop proliferating and remain in the G_0_ and G_1_ phases of the cell cycle. In combination with other therapeutic agents or alone, TAM has also been shown to be antiangiogenic, which is, at least in part, independent of its ER-antagonist properties (7). TAM also has a number of other beneficial properties. For example, TAM lowers low-density lipoprotein cholesterol levels, increases bone density in postmenopausal women, and is effective against infertility in women with anovulatory disorders. In men, TAM is used to treat breast cancer, and it is also used to treat gynecomastia that arises from anti-androgen treatment in patients with prostate cancer.

TAM has some side effects. It blocks the estrogen effects on mammary epithelial cells, but it mimics the estrogen actions in other tissues (2). The result of such selective effects on the uterus is stimulated proliferation of the endometrium (8). Each year, the risk of developing endometrial cancer (http://www.cancer.gov/cancertopics/factsheet/Therapy/tamoxifen) is ~2‰ in women taking TAM compared with ~1‰ in women taking placebo (9). TAM also slightly increases the risk of developing uterine sarcoma (http://www.cancer.gov/clinicaltrials/results/tamoxifen-and-uterine-sarcoma0502). The other side effects include blood clots, strokes, cataracts, and symptoms of menopause. To maintain the beneficial properties without sharing the potentially harmful effects of TAM, a number of derivatives have been developed (2). However, these derivatives demonstrate differing amounts of success. Their ability to inhibit cancer ranges widely.

Studies of tissue-based pharmacokinetics of TAM and its derivatives provide direct concentration-effect relationships in tumors and critical normal tissues, thus providing a more rational basis for the evaluation of new compounds and tumor response to treatment (10, 11). Generally speaking, the study results are controversial. Imaging studies have shown that [^18^F]fluorotamoxifen is useful in predicting the effect of TAM therapy in patients with ER-positive breast cancer (12, 13). The ^123^I-trans-Z-iodomethyl-N,N-diethyltamoxifen has also been shown to be preferentially taken up by ER-positive tumors in patients with untreated primary breast cancer (14, 15). On the contrary, studies have failed to show the suitability for tumor localization of some derivatives, such as ^131^I- and ^99m^Tc-labeled geometrical isomers (E and Z) of the aminotamoxifen, ^125^I-idoxifene and ^11^C-toremifene (16-19). Recently, Muftuler et al. produced ^131^I-TAM and investigated its biodistribution in rats. Their study demonstrated that the biodistribution of ^131^I-TAM is ER-specific (3).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tamoxifen+cancer+biodistribution%20AND%20synthesis)]

The synthesis of ^131^I-TAM was based on the oxidation of iodide by iodogen as described in detail by Muftuler et al. (3). Briefly, four reaction vials of iodogen in CH_2_Cl_2_ solution (100 µg (578.6 nmol/ml)) were prepared and evaporated separately to form a thin solid layer of iodogen on the wall of each reaction vial. TAM (1 ml, 0.54 µmol/ml) and Na^131^I (0.4 ml, 185 MBq (5 mCi)) were added to the first reaction vial. The mixture (pH 8.0) was gently mixed and incubated for 5 min at room temperature. The reaction solution was then successively transferred to the other three vials with incubation in each vial for 5 min at room temperature. As the final step, 0.1 ml Na_2_SO_3_ solution (0.1 N) was added to the last vial to reduce the unincorporated iodine. Radioelectrophoresis revealed that ^131^I-TAM had a neutral structure at room temperature. Structural analysis showed that stable ^127^I was attached to TAM in the ortho position of the aromatic ring containing the ether group. The product yield and the specific activity of ^131^I-TAM were 88.56 ± 3.10% and 0.53 GBq/μmol (14.32 mCi/μmol), respectively (n = 8 replicates). The purity of ^131^I-TAM was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tamoxifen%20cancer%20biodistribution%20AND%20in%20vitro)]

The stability of ^131^I-TAM was analyzed in vitro by incubation with human serum at 37ºC for different times. It was shown that ~45% of the ^131^I-TAM existed as an intact complex in human serum within 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=tamoxifen%20cancer%20biodistribution%20AND%20animal)]

Muftuler et al. investigated the biodistribution of ^131^I-TAM in healthy female Albino Wistar rats weighing 130–180 g (3). A total of 7.4 MBq (200 μCi) ^131^I-TAM was given to each rat via the tail vein. The animals were euthanized at 30, 60, and 180 min (n = 3 animals/time point), and the accumulated radioactivity in each organ was measured. To block the iodine uptake by the thyroid gland, potassium iodide was added to the animals’ drinking water. To determine whether the uptake of ^131^I-TAM in tissues was ER-specific, an ER-blocking experiment was performed by administration of 4.4 µg (11.84 nmol) of the non-labeled TAM to each rat through the tail vein 15 min before the injection of ^131^I-TAM. The non-labeled TAM was prepared under the same conditions as the ^131^I-TAM.

The detailed biodistribution data were reported by Muftuler et al. (Table 3) (3). In animals without ER blocking, uptake of ^131^I-TAM in all ER-rich tissues was considerably high at the time points examined. Analysis of the blood samples suggested that the biological half-life of ^131^I-TAM was ~11 h, which was shorter than the physical half-life of ^131^I (8.02 days). In the uterus, the ^131^I-TAM reached the maximum level of accumulation (15.66 ± 0.76% injected dose per gram (ID/g)) within 30 min after injection, and it remained in the uterus within 180 min. Uptake of the ^131^I-TAM in this study was faster than that of estrogen derivatives in other reports (3). The uterus/blood and uterus/muscle uptake ratios at 30 min were ~1 and ~3, respectively. The ^131^I-TAM level in the uterus was three times higher in animals without ER blocking than in animals with ER blocking (5.74 ± 0.48% ID/g). The kidney, as the primary organ of metabolism and excretion of estrogen, showed a high uptake of ^131^I-TAM. The uptake level increased within 60 min (22.83 ± 4.86% ID/g at 60 min) after injection, followed by a rapid decrease. The lung is known to have a specific affinity for all kinds of amines. Consistent with that, a high level of ^131^I-TAM uptake (15.81 ± 3.3% ID/g at 30 min) was observed in the lung without ER blocking. The ^131^I-TAM level at 180 min was two times higher in the lung without ER blocking (11.06 ± 3.43% ID/g) than in the lung with blocking (4.04 ± 1.68% ID/g). Differences in tissue uptake levels between animals without and with ER blocking were also significant (P < 0.05) for heart, liver, kidneys, small intestine, large intestine, muscle, and fat tissue.

An imaging study was also performed with female rats weighing 150–200 g (n = 6) with the use of an e-Cam Single Camera equipped with a low-energy high-resolution collimator (3).. ^131^I-TAM (~9.6 MBq (~260 μCi)/rat) was administered via the tail vein. To block the ER, 10 μg (26.92 nmol) of non-labeled TAM was given to each rat through the tail vein 15 min before injection with ^131^I-TAM. Imaging showed that the stomach had the highest uptake among all organs. The uptake level increased over time. The ratio of radioactivity in the stomach without ER blocking to radioactivity in the stomach with ER blocking was ~1.5 at both 30 and 60 min. The uptake levels in the liver and gastrointestinal tract were low. Detailed imaging data were not shown for other organs, including uterus and breast.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Vogel V.G. (2009). The NSABP Study of Tamoxifen and Raloxifene (STAR) trial. Expert Rev Anticancer Ther.
2 Oseni T., Patel R., Pyle J., Jordan V.C. (2008). Selective estrogen receptor modulators and phytoestrogens. Planta Med.
3 Muftuler F.Z., Unak P., Teksoz S., Acar C., Yolcular S., Yurekli Y. (2008). 131I labeling of tamoxifen and biodistribution studies in rats. Appl Radiat Isot.
4 Sommer S., Fuqua S.A. (2001). Estrogen receptor and breast cancer. Semin Cancer Biol.
5 Higgins M.J., Rae J.M., Flockhart D.A., Hayes D.F., Stearns V. (2009). Pharmacogenetics of tamoxifen: who should undergo CYP2D6 genetic testing?. J Natl Compr Canc Netw.
6 Goetz M.P., Rae J.M., Suman V.J., Safgren S.L., Ames M.M., Visscher D.W., Reynolds C., Couch F.J., Lingle W.L., Flockhart D.A., Desta Z., Perez E.A., Ingle J.N. (2005). Pharmacogenetics of tamoxifen biotransformation is associated with clinical outcomes of efficacy and hot flashes. J Clin Oncol.
7 Banerjee S., Dowsett M., Ashworth A., Martin L.A. (2007). Mechanisms of disease: angiogenesis and the management of breast cancer. Nat Clin Pract Oncol.
8 Kim K.H., Bender J.R. (2009). Membrane-initiated actions of estrogen on the endothelium. Mol Cell Endocrinol.
9 Polin S.A., Ascher S.M. (2008). The effect of tamoxifen on the genital tract. Cancer Imaging.
10 Young H., Carnochan P., Trivedi M., Potter G.A., Eccles S.A., Haynes B.P., Jarman M., Ott R.J. (1995). Pharmacokinetics and biodistribution of radiolabelled idoxifene: prospects for the use of PET in the evaluation of a novel antioestrogen for cancer therapy. Nucl Med Biol.
11 Van de Wiele C., Cocquyt V., VandenBroecke R., De Vos F., Van Belle S., Dhaene K., Slegers G., Dierckx R.A. (2001). Iodine-labeled tamoxifen uptake in primary human breast carcinoma. J Nucl Med.
12 Inoue T., Kim E.E., Wallace S., Yang D.J., Wong F.C., Bassa P., Cherif A., Delpassand E., Buzdar A., Podoloff D.A. (1996). Positron emission tomography using [18F]fluorotamoxifen to evaluate therapeutic responses in patients with breast cancer: preliminary study. Cancer Biother Radiopharm.
13 Inoue T., Kim E.E., Wallace S., Yang D.J., Wong F.C., Bassa P., Buzdar A.U., Podoloff D.A. (1997). Preliminary study of cardiac accumulation of F-18 fluorotamoxifen in patients with breast cancer. Clin Imaging.
14 De Vos F., Van de Wiele C., Vandecapelle M., Dierckx R.A., Slegers G. (2001). High performance liquid chromatographic determination of 123-I labeled tamoxifen metabolites in human plasma. Nucl Med Biol.
15 Van de Wiele C., De Vos F., De Sutter J., Dumont F., Slegers G., Dierckx R.A., Thierens H. (1999). Biodistribution and dosimetry of (iodine-123)-iodomethyl-N, N-diethyltamoxifen, an (anti)oestrogen receptor radioligand. Eur J Nucl Med.
16 Delpassand E.S., Yang D.J., Wallace S., Cherif A., Quadri S.M., Price J., Joubert A., Inoue T., Podoloff D.A. (1996). Synthesis, biodistribution, and estrogen receptor scintigraphy of indium-111-diethylenetriaminepentaacetic acid-tamoxifen analogue. J Pharm Sci.
17 Hunter D.H., Luyt L.G. (2000). Single isomer technetium-99m tamoxifen conjugates. Bioconjug Chem.
18 Kangas L., Haaparanta M., Paul R., Roeda D., Sipila H. (1989). Biodistribution and scintigraphy of 11C-toremifene in rats bearing DMBA-induced mammary carcinoma. Pharmacol Toxicol.
19 Strickland L.A., Ponce Y.Z., Hunter D.H., Zabel P.L., Powe J.E., Morrissey G., Driedger A.A., Chamberlain M.J., Tustanoff E.R. (1990). Amino and iodotamoxifens: synthesis, estrogen receptor affinity and biodistribution. Drug Des Deliv.